# Gadolinium-diethylenetriamine pentaacetic acid-carboxymethylarabinogalactan

Chemical name: | Gadolinium-diethylenetriamine pentaacetic acid- carboxymethylarabinogalactan
Abbreviated name: | Gd-DTPA-CMAG-A_2_
Synonym:
Agent category: | Polysaccharide
Target: | Hepatic asialoglycoprotein receptor (ASGP-R)
Target category: | Receptor
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal/contrast: | Gadolinium, Gd
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gd-CMAG)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used in imaging because of their abundance in water molecules. Water comprises ~80% of most soft tissue. The contrast of proton MRI depends primarily on the density of the nucleus (proton spins), the relaxation times of the nuclear magnetization (T1, longitudinal; T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the development of contrast agents. Most contrast agents affect the T1 and T2 relaxation times of the surrounding nuclei, mainly the protons of water. T2* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (1). Cross-linked iron oxide (CLIO) nanoparticles and other iron oxide formulations affect T2 primarily and lead to decreased signals. On the other hand, paramagnetic T1 agents such as gadolinium (Gd^3+^) and manganese (Mn^2+^) accelerate T1 relaxation and lead to increased contrast images.

Gd, a lanthanide metal ion with seven unpaired electrons, has been shown to be very effective in enhancing proton relaxation because of its high magnetic moment and water coordination (2, 3). Gd-labeled diethylenetriaminepentaacetic acid (Gd-DTPA) was the first intravenous MRI contrast agent used clinically, and a number of similar Gd chelates have been developed in an effort to further improve clinical use. However, these low molecular weight Gd chelates have short blood and tissue retention times, which limit their use as imaging agents in the vasculature and in cancer tissues. Furthermore, they are largely nonspecific. Arabinogalactan, a polysaccharide, binds specifically to hepatocytes via asialoglycoprotein receptor (ASGP-R) (4-6). Li et al. (7) prepared aminated carboxymethylarabinogalactan (CMAG-A_2_) to link with Gd-DTPA to form Gd-DTPA-CMAG-A_2_ for imaging the liver via ASGP-R.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gd-CMAG+synthesis)]

DTPA-CMAG-A_2_ was prepared by incubation of DTPA succinimide ester (~14 mmol) and CMAG-A_2_ (0.51 mmol) (pH 10) at room temperature for 24 h (7). GdCl_3_•6 H_2_O was added to the solution of DTPA-CMAG-A_2_ (1.2:1 molar ratio) and incubated at room temperature for 18–20 h. The product, Gd-DTPA-CMAG-A_2_, was isolated with column chromatography. DTPA-CMAG-A_2_ had 0.51 mmol of DTPA/g.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gd-CMAG+in+vitro)]

Gd-DTPA-CMAG-A_2_ and Gd-DTPA exhibited T1 relaxivity r_1_ values (0.47 T) of 7.9 and 5.4 mM^-1^s^-1^ at 37°C in buffer containing bovine serum albumin, respectively (7). The r_1_ value of Gd-DTPA-CMAG-A_2_ was not affected by the addition of equal molar of Ca^2+^ or ethylenediaminetetraacetic acid.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gd-CMAG+rodentia)]

Li et al. (7) performed dynamic T1-weighted MRI imaging (4.7 T) studies in rats (n = 3) after injection of Gd-DTPA-CMAG-A_2_ (79 nmol/kg) or Gd-DTPA (96 nmol/kg). The mean enhancement of the liver parenchyma and kidney was 38.7 ± 6.4% and 69.4 ± 4.4% for Gd-DTPA-CMAG-A_2_ at 10–30 min, respectively. On the other hand, the mean enhancement of the liver parenchyma and kidney was 21.9 ± 4.5% and 53.8 ± 4.8% for Gd-DTPA at 10–30 min, respectively. The hepatic uptake rate of Gd-DTPA-CMAG-A_2_ (half-life (t_1/2_), 0.8 min) was faster than that of Gd-DTPA (t_1/2_, 16.7 min), whereas the liver excretion rate of Gd-DTPA-CMAG-A_2_ (t_1/2_, 129.8 min) was slower than that of Gd-DTPA (t_1/2_, 52.4 min). The renal uptake rate of Gd-DTPA-CMAG-A_2_ (t_1/2_, 0.1 min) was faster than that of Gd-DTPA (t_1/2_, 4.6 min), whereas the renal excretion rate of Gd-DTPA-CMAG-A_2_ (t_1/2_,153.8 min) was slower than that of Gd-DTPA (t_1/2_, 86.1 min). Rats receiving Gd-DTPA-CMAG-A_2_ exhibited increases in the MR signal intensity in the liver comparing with Gd-DTPA at 10-90 min after injection. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gd-CMAG+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gd-CMAG+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Gd-CMAG+human)]

No publication is currently available.

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 Brasch R.C. (1992). New directions in the development of MR imaging contrast media. Radiology.
3 Runge V.M., Gelblum D.Y. (1991). Future directions in magnetic resonance contrast media. Top Magn Reson Imaging.
4 Gallez B., Lacour V., Demeure R., Debuyst R., Dejehet F., De Keyser J.L., Dumont P. (1994). Spin labelled arabinogalactan as MRI contrast agent. Magn Reson Imaging.
5 Groman E.V., Enriquez P.M., Jung C., Josephson L. (1994). Arabinogalactan for hepatic drug delivery. Bioconjug Chem.
6 Prata M.I., Santos A.C., Torres S., Andre J.P., Martins J.A., Neves M., Garcia-Martin M.L., Rodrigues T.B., Lopez-Larrubia P., Cerdan S., Geraldes C.F. (2006). Targeting of lanthanide(III) chelates of DOTA-type glycoconjugates to the hepatic asyaloglycoprotein receptor: cell internalization and animal imaging studies. Contrast Media Mol Imaging.
7 Li W., Li Z., Jing F., Deng Y., Wei L., Liao P., Yang X., Li X., Pei F., Wang X., Lei H. (2008). Synthesis and evaluation of Gd-DTPA-labeled arabinogalactans as potential MRI contrast agents. Carbohydr Res.